# [^149/152/155/161^Tb]-Labeled DOTA-folate conjugated to an albumin-binding entity

Chemical name: | [^149/152/155/161^Tb]-Labeled DOTA-folate conjugated to an albumin-binding entity
Abbreviated name: | [^149/152/155/161^Tb]cm09
Synonym:
Agent Category: | Peptide
Target: | Folate receptor (FR)
Target Category: | Receptor
Method of detection: | Positron emission tomography (PET); single-photon emission computed tomography (SPECT) and gamma planar imaging
Source of signal / contrast: | ^149/152/155/161^Tb
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Folate%20receptor&cmd=DetailsSearch)]

The folate receptor (FR) is overexpressed in several types of neoplastic tumors and in activated macrophages that accumulate at the site(s) of inflammation (1). As a consequence, the FR is targeted with different types of radiolabeled probes (usually derivatives of folate) to visualize cancerous lesions or inflammation with noninvasive imaging techniques [MICAD (http://www.ncbi.nlm.nih.gov/books/?term=folate+receptor+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)]. Positron emission computed tomography (PET) and single-photon emission computed tomography (SPECT) are the most common imaging modalities that have been used to detect these pathologies with the radiolabeled folate derivatives, and radionuclides such as ^18^F or ^68^Ga (for PET) and ^99m^Tc or ^111^In (for SPECT) are usually used to generate the probes. In addition, compounds radiolabeled with ^177^Lu, ^188^Re, or ^67^Cu (all visualized with SPECT) that target the FR have been shown to be useful for the radiotherapy of cancers that overexpress this receptor (1). A major limitation of using the above-mentioned radionuclides for the detection or radiotherapy of cancers in the clinic is the availability and cost of producing these radioactive isotopes. The ideal radionuclides that can be used to detect and treat cancers would be those that are produced from the same source in a short time, have a sufficiently long half-life, and can be easily incorporated into a compound to generate a radiolabeled imaging probe.

Terbium (Tb; a lanthanide), has four radioisotopes (^149/152/155/161^Tb) that are considered to be clinically relevant because of their half-lives, energies, and decay properties as described in Table 1 (2). It was suggested that the ^152^Tb isotope was probably suitable to study the kinetics of radiolanthanides with PET (3), and the ^149^Tb isotope was used successfully to label retuximab for the radiotherapy of human xenograft tumors that express the CD20 antigen in mice (4). In another study, it was shown that the decay characteristics and the production parameters for the ^161^Tb isotope are similar to those for ^177^Lu and that ^161^Tb can be produced in sufficient quantities to label compounds that are to be used for radiotherapy (5). Therefore, the different isotopes of Tb are considered to be appropriate for the generation of radiolabeled probes or radioconjugates because they would have identical structural and chemical properties and could be used as matched pairs either for nuclear imaging or for the radiotherapy of different diseases.

A unique 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (DOTA) conjugate of folic acid containing an albumin-binding entity (cm09) was synthesized and labeled with the different isotopes of Tb (2). Each component of cm09 has an exclusive functional attribute that contributes to the biological and imaging properties of the intact molecule. The folic acid moiety targets the molecule to the FR, cm09 increases the blood circulation time of the molecule by binding to plasma proteins, and DOTA chelates the radionuclide that generates the signal for imaging. In addition, the prolonged circulation time of the molecule corresponds with the half-lives of the longer-living Tb radioisotopes (see Table 1) (2). A [177Lu] conjugate of cm09 has been shown to generate a high tumor-to-kidney ratio in mice and was suggested to be suitable for folic acid-targeted radionuclide therapy of cancerous tumors in rodents (6). For proof of concept studies, the cm09 molecule was labeled with each one of the Tb isotopes (^149/152/155/161^Tb), and the biodistribution of [^161^Tb]cm09 was studied in mice bearing KB cell (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CCL-17&Template=cellBiology) tumors, which express the FR. In another study, [^152^Tb]cm09 and [^155/161^Tb]cm09 were evaluated with PET and SPECT, respectively, for the detection of KB cell lesions in the animals (2). In addition, the efficacies of the [^149/161^Tb]cm09 conjugates were investigated for the treatment of cancerous tumors in the rodents.

### Related Resource Links

FR-related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=folate+receptor+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Human mRNA (http://www.ncbi.nlm.nih.gov/nuccore?term=%28Human%20human%20folate%20receptor%29%20AND%20%22Homo%20sapiens%22%5bporgn%3A__txid9606%5d&cmd=DetailsSearch) and protein (http://www.ncbi.nlm.nih.gov/protein/AAB05827.1) sequences of FR

FR in Online Mendelian Inheritance in Man database (OMIM (http://omim.org/entry/136430))

Folate pathway in humans (from Kyoto Encyclopedia of Genes and Genomes (KEGG (http://www.genome.jp/kegg-bin/show_pathway?hsa04144)))

FR-related clinical trials (http://clinicaltrials.gov/ct2/results?term=Folate+receptor&Search=Search)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=DOTA-folate-cm09&cmd=DetailsSearch)]

The ^149/152/155/161^Tb radioisotopes used in the various studies were produced as described by Muller et al. (2). The cm09 molecule was labeled with the different radioisotopes of Tb (2). The radiochemical yield, radiochemical purity, and specific activity of the different radiolabeled conjugates of cm09 are given in Table 2.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=DOTA-folate-cm09&cmd=DetailsSearch)]

Radiolysis of [^161^Tb]cm09 was investigated by incubating the tracer (80 MBq, 2 nmol) in phosphate-buffered saline (PBS, pH 7.4) for up to 48 h (incubation conditions not reported) (2). Samples were obtained from the incubation mix at various time points and analyzed with high-performance liquid chromatography (HPLC). No radiolysis was detected for up to 4 h of incubation, but a single peak of unknown composition constituting ~5% of the integrated peak area appeared at 24 h and increased to ~7% after 48 h. No free Tb was detected during the entire period of incubation.

[^161^Tb]cm09 was reported to be completely stable in human plasma at 37°C for up to 168 h as determined with HPLC analysis (2).

The cell binding and internalization characteristics of [^161^Tb]cm09 were studied by incubating the radiochemical with KB cells (these cells have a high expression of FR) at 37°C for up to 4 h (2). After 4 h, ~65% of added radioactivity from [^161^Tb]cm09 was observed to bind to the FR-expressing KB cells, and ~30% of the radioactivity was internalized by the cells. Preincubation of the cells with excess folic acid (100 μM) reduced the binding to <1% of added radioactivity. This indicated that [^161^Tb]cm09 had a high binding specificity for the FR.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=DOTA-folate-cm09&cmd=DetailsSearch)]

The biodistribution of [^161^Tb]cm09 was studied in nude mice bearing KB cell xenograft tumors (2). Each mouse (number of animals per time point not reported) was administered with ~3 MBq (~111 μCi, 0.5 nmol) [^161^Tb]cm09 through the lateral tail vein, and the animals were euthanized at predetermined time points to harvest the organs of interest to determine the amount of radioactivity accumulated in the various tissues. Results obtained from this study were presented as percent of injected dose per gram tissue (% ID/g). At all the time points, maximum uptake of radioactivity was observed in the kidney (Table 3), followed by the tumor and the liver. The tumor/blood ratio increased from 1.2 ± 0.1 at 1 h postinjection (p.i.) to 129.4 ± 18.0 at 168 h p.i. The tumor/liver ratio was 2.6 ± 0.2 at 1 h p.i., increased to 5.9 ± 0.6 at 24 h p.i., and remained relatively constant thereafter. The tumor/kidney ratio was the highest at 4 h p.i. (0.87 ± 0.12) and remained almost constant for up to 168 h p.i. No blocking studies were reported.

Mice bearing KB cell tumors (n = 2 animals) were injected with ~9 MBq (333 μCi, 6.8 nmol) [^152^Tb]cm09 as before to evaluate the use of this radiochemical for the PET imaging of cancerous lesions (2). The rodents were euthanized at 24 h p.i., and whole-body PET scans of the animals were acquired for 4 h. Each PET scan was immediately followed with computed tomography (CT), and images obtained with the two imaging modalities were reconstructed with appropriate software. The tumors and the kidneys were clearly visible in the reconstructed PET/CT images of the animals. Almost no accumulation of radioactivity was observed in all other organs and tissues. No blocking studies were reported.

In another study, mice bearing KB cell tumors (n = 2 animals/tracer) were injected with either ~4 MBq (148 μCi; 6.3 nmol) [^155^Tb]cm09 or ~30 MBq (1.11 mCi, 1.1 nmol) [^161^Tb]cm09 as before to evaluate the use of these radiochemicals for the SPECT imaging of neoplastic lesions (2). Whole-body SPECT images of the animals were acquired with a small animal SPECT/CT scanner as described elsewhere (2). Each SPECT scan was followed with a CT scan, and images acquired with the two imaging modalities were reconstructed using appropriate software. The tumors and the kidneys were clearly visible in the reconstructed SPECT/CT images obtained with both radiochemicals. Almost no radioactivity was detected in the other organs and tissues of the animals with either tracer. No blocking studies were reported.

KB cell tumor bearing mice were used to investigate the radiotherapeutic potential of [^149^Tb]cm09 and [^161^Tb]cm09 as described by Muller et al. (2). For [^149^Tb]cm09, the rodents (n = 3 animals/group) were injected on two separate days either with PBS (group a, controls; injections were given on day 0 and on day 4) or [^149^Tb]cm09 (group b; 1.1 MBq (40.7 μCi, ~4 nmol) on day 0 and 1.3 MBq (48.1 μCi, ~4 nmol) on day 4). For the study with [^161^Tb]cm09, the animals (n = 5 mice/group) were injected only once either with PBS (group c, controls) or [^161^Tb]cm09 (group d; 11 MBq (407 μCi, ~4 nmol)). The groups of animals were observed for up to 56 d p.i. In group a, all mice showed a rapid growth of the tumors, whereas in comparison the lesions were reported to grow slowly in animals that received the two injections of [^149^Tb]cm09 (group b). In group b, only one animal showed complete regression of the tumor, but in the other two animals the tumors started to regrow after several days. All mice treated with [^161^Tb]cm09 (group d) showed reduced tumor growth compared with the control animals (group c). In group d, only one animal showed tumor escape, and the other four mice exhibited complete tumor regression. Mice treated with [^149^Tb]cm09 or [^161^Tb]cm09 showed a significantly longer survival time compared with the control animals (P values for [^149^Tb]cm09 and [^161^Tb]cm09 were <0.05 and <0.005, respectively).

From these studies, the investigators concluded that the Tb radioisotopes were suitable to produce multiple radioconjugates that could be used for different applications; however, more extensive preclinical studies were necessary to confirm that they can be used in the clinic for the detection and treatment of cancerous tumors (2).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=DOTA-folate-cm09%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No reference is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=DOTA-folate-cm09%20Non-Human%20Primates&cmd=DetailsSearch)]

No reference is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=DOTA-folate-cm09%20Human%20Studies&cmd=DetailsSearch)]

No reference is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Muller C. (2012). Folate based radiopharmaceuticals for imaging and therapy of cancer and inflammation. Curr Pharm Des.
2 Muller C., Zhernosekov K., Koster U., Johnston K., Dorrer H., Hohn A., van der Walt N.T., Turler A., Schibli R. (2012). A Unique Matched Quadruplet of Terbium Radioisotopes for PET and SPECT and for alpha- and beta--Radionuclide Therapy: An In Vivo Proof-of-Concept Study with a New Receptor-Targeted Folate Derivative. J Nucl Med.
3 Allen B.J., Goozee G., Sarkar S., Beyer G., Morel C., Byrne A.P. (2001). Production of terbium-152 by heavy ion reactions and proton induced spallation. Appl Radiat Isot.
4 Beyer G.J., Miederer M., Vranjes-Duric S., Comor J.J., Kunzi G., Hartley O., Senekowitsch-Schmidtke R., Soloviev D., Buchegger F. (2004). Targeted alpha therapy in vivo: direct evidence for single cancer cell kill using 149Tb-rituximab. Eur J Nucl Med Mol Imaging.
5 Lehenberger S., Barkhausen C., Cohrs S., Fischer E., Grunberg J., Hohn A., Koster U., Schibli R., Turler A., Zhernosekov K. (2011). The low-energy beta(-) and electron emitter (161)Tb as an alternative to (177)Lu for targeted radionuclide therapy. Nucl Med Biol.
6 Muller, C., H. Struthers, C. Winiger, K. Zhernosekov, and R. Schibli, DOTA Conjugate with an Albumin-Binding Entity Enables the First Folic Acid-Targeted 177Lu-Radionuclide Tumor Therapy in Mice. J Nucl Med, 2012

Table 1: Properties of Terbium radioisotopes (2).

Radionuclide | Decay mode and branching | Half-life (t _ 1/2 _ ) | Clinical application
^ 149 ^ Tb | α (16.7%) β^+^ (7.1%) | 4.12 h | α-therapy
^ 152 ^ Tb | β^+^ (17.0%) | 17.50 h | PET
^ 155 ^ Tb | EC* (100%) | 5.32 d | SPECT
^ 161 ^ Tb | β^–^ (100%) | 6.89 d | β^–^/auger therapy

* Electron capture; The E_γ_ value are 86.55, 105.3, 180.1 and 262.3, respectively. The I_γ_ (%) for the

E_γ_ values are 32, 25, 7.5 and 5.3, respectively.

Table 2: Radiochemical yield, radiochemical purity, and specific activity of [^149/152/155/161^Tb]cm09 (2).

Radiolabeled cm09 | Radiochemical yield | Radiochemical purity | Specific activity
[ ^ 149 ^ Tb]cm09 | >96% | >96% | ~0.48 MBq/nmol (~17.76 μCi/nmol)
[ ^ 152 ^ Tb]cm09 | >96% | >96% | ~1.33 MBq/nmol (~49.0 μCi/nmol)
[ ^ 155 ^ Tb]cm09 | >96% | >96% | ~0.64 MBq/nmol (~23.7 μCi/nmol)
[ ^ 161 ^ Tb]cm09 | >98% | >98% | ~40.0 MBq/nmol (~1.48 mCi/nmol)

Table 3: Biodistribution of radioactivity from [^161^Tb]cm09 in nude mice bearing KB cell tumors.

Organ | Time postinjection (h)
Organ | 1 | 4 | 24 | 48 | 96 | 168
Organ | Percent of injected dose per gram tissue
Blood | 11.2 ± 1.1 | 6.1 ± 0.3 | 1.5 ± 0.1 | 0.72 ± 0.18 | 0.16 ± 0.01 | 0.04 ± 0.01
Kidneys | 20.5 ± 2.7 | 27.5 ± 1.1 | 27.8 ± 5.0 | 24.5 ± 1.6 | 15.5 ± 3.2 | 7.4 ± 1.7
Liver | 5.5 ± 0.3 | 5.1 ± 0.6 | 3.8 ± 0.7 | 2.3 ± 0.4 | 1.6 ± 0.2 | 0.86 ± 0.16
Muscle | 1.8 ± 0.1 | 1.9 ± 0.2 | 1.3 ± 0.1 | 0.70 ± 0.03 | 0.45 ± -.06 | 0.16 ± 0.08
Tumor | 14.1 ± 0.6 | 23.8 ± 2.5 | 22.0 ± 4.4 | 18.5 ± 1.8 | 10.3 ± 1.8 | 5.7 ± 1.9
Tumor/blood | 1.2 ± 0.1 | 3.9 ± 0.3 | 14.3 ± 2.0 | 26.8 ± 6.5 | 64.7 ± 8.4 | 129.4 ± 18.0
Tumor/liver | 2.6 ± 0.2 | 4.7 ± 0.5 | 5.9 ± 0.6 | 8.1 ± 1.7 | 6.5 ± 1.7 | 6.5 ± 1.2
Tumor/kidney | 0.68 ± 0.07 | 0.87 ± 0.12 | 0.79 ± 0.05 | 0.75 ± 0.04 | 0.70 ± 0.09 | 0.76 ± 0.12

For complete data see Muller et al. (2).